# (S,S)-2-(α-(2-[^18^F]Fluoro[^2^H_2_]methoxyphenoxy)phenoxy)benzyl)morpholine

Chemical name: | (S,S)-2-(α-(2-[^18^F]Fluoro[^2^H_2_]methoxyphenoxy)benzyl)morpholine
Abbreviated name: | (S,S)-[^18^F]FMeNER-D_2_
Synonym: | (S,S)-[^18^F]MRB
Agent Category: | Compound
Target: | Brain norepinephrine transporter (NET)
Target Category: | Transporter binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal/contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B18F%5DFMeNER%20OR%2018F-Reboxetine%20analog)]

(S,S)-2-(α-(2-[^18^F]Fluoro[^2^H_2_]methoxyphenoxy)benzyl)morpholine ((S,S)-[^18^F]FMeNER-D_2_) is a radioligand developed for positron emission tomography (PET) imaging of the brain adrenergic receptors. It is a derivative of reboxetine ((RS)-2-[(RS)-2-ethoxyphenoxy)benzyl]morpholine), a norepinephrine transporter (NET) inhibitor, labeled with ^18^F, a positron emitter with a physical half-life (t_½_) of 109.8 min (1, 2).

Many diseases affect the sympathetic nervous system (SNS), and imaging of pathologic changes of adrenergic transmission has been an important area of PET research (3, 4). Most postganglionic sympathetic neurons in the autonomic nervous system release the neurotransmitter norepinephrine (NE), which stimulates adrenergic receptors in various effector organs (5). There are different types and subtypes of adrenergic receptors, and they are characterized as α_1a_ to α_1c_, α_2a_ to α_2c_, and β_1_ to β_3_ (6). All of the NE receptors belong to the G-protein-linked receptor superfamily and mediate slow neuromodulatory postsynaptic responses. The NET is a transmembrane protein located in the adrenergic nerve terminals that is responsible for active reuptake (uptake-1) of NE released from neurons (7). NE is stored in the neuronal vesicles and is released on stimulation. Significant expression of NET is found in major organs of the SNS, such as the heart and brain. Brain NETs are involved in various neurologic and psychiatric diseases, including depression, attention deficit hyperactivity disorder, drug addiction, and eating disorders (8). Brain NETs are also the site of action of many antidepressant drugs in the brain (9).

Molecular probes with structures closely related to NE can be used to assess the integrity of presynaptic sympathetic nerve terminals in various diseases. In vivo NE synthesis is similar to dopamine synthesis, and dopamine is converted to NE by the enzyme dopamine-β-hydroxylase (6). [^123^I]-meta-Iodobenzylguanidine, [^11^C]m-hydroxyephedrine, [^11^C]norepinephrine, and many other radioligands have been developed and used for peripheral neuronal imaging (10). However, this class of tracers is not suitable for the study of brain NET system because they are not able to cross the blood-brain barrier (11). In the brain, NET levels are relatively lower than other receptors, such as dopamine transporters (DATs) and serotonin transporters. (9). Several NET reuptake inhibitors, such as [^11^C]desipramine, have been tested, but they showed high nonspecific binding. Reboxetine is a specific NET inhibitor with a high affinity and selectivity (inhibitory concentration (IC_50_) DAT/NET = 4,000). The (S,S)-MeNER enantiomer ((S,S)-MRB) is the more potent enantiomer with a IC_50_ of 3.6 nM for inhibiting NE uptake in rat hypothalamic synaptosomes. ^11^C-labeled (S,S)-MeNER has been shown to be a promising brain NET imaging agent, but the specific binding peak equilibrium could not be measured because of the short t_½_ of ^11^C. Because of the longer t_½_ of ^18^F, Shou et al. (1) described the synthesis of the first radiofluorinated ligand, (S,S)-[^18^F]FMeNER, for brain NET imaging. The di-deuterated analog, (S,S)-[^18^F]FMeNER-D_2_, was developed to minimize the in vivo defluorination of (S,S)-[^18^F]FMeNER (1).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFMeNER%20OR%2018F-Reboxetine%20analog%29%20AND%20synthesis)]

(S,S)-[^18^F]FMeNER-D_2_ was prepared by O-fluoromethylation of the precursor, desfluoromethoxy-(S,S)-FMeNER, with [^18^F]fluorobromomethane-d_2_ (1). [^18^F]fluorobromomethane-d_2_ was prepared from [^18^F]fluoride ion (12). In this procedure, [^18^F]fluoride was isolated from a Sep-Pak QMA cartridge elution and was then reacted with dibromomethane-d_2_ in acetonitrile at 90 °C for 10-15 min. Desfluoromethoxy-(S,S)-FMeNER was reacted with [^18^F]bromofluoromethane-d_2_ in N,N-dimethylformamide at 90 °C for 5 min. (S,S)-[^18^F]FMeNER-D_2_ was purified by reverse-phase high-performance liquid chromatography. An alternative method involved reaction of [^18^F]fluoromethyl-d_2_ triflate with the N-Boc-protected precursor. The mixture was heated at 90 °C for 4 min.

The yield of [^18^F]fluorobromomethane-d_2_ was between 15 and 25% (noncorrected), and the subsequent yield of (S,S)-[^18^F]FMeNER-D_2_ was >90%. The overall yield of (S,S)-[^18^F]FMeNER-D_2_ from [^18^F]fluoride was between 5 and 10% with a total synthesis time of about 75 min. The radiochemical purity was >98%, and the specific activity at time of injection was about 111-185 GBq/μmol (3,000-5,000 Ci/mmol) in 0.08-0.2 μg of (S,S)-[^18^F]FMeNER-D_2_. The radioligand was stable in the phosphate-buffered saline formulation for the duration of the experiments. Radiochemical purity was >95% at 5 h after formulation.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFMeNER%20OR%2018F-Reboxetine%20analog%29%20AND%20in%20vitro)]

Schou et al. (1, 13) performed in vitro autoradiography in human brains by incubating human brain sections with 4 MBq (0.11 mCi) of (S,S)-[^18^F]FMeNER-D_2_ for 90 min at room temperature. The study showed that (S,S)-[^18^F]FMeNER-D_2_ bound substantially to the cerebral and cerebellar gray matter but that binding to the white matter was lower. The binding was highest in the locus coeruleus. Lower binding was observed in the cerebellum, temporal cortex, and thalamus. The binding, expressed as percentage of locus coeruleus binding, was 15.2, 12.3, and 8.0 in the cerebellum, temporal cortex, and thalamus, respectively. This binding was blocked by 10 μM desipramine (selective NET inhibitor), but no inhibition was observed with the DAT inhibitor PE2I or the serotonin transporter inhibitor citalopram.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFMeNER%20OR%2018F-Reboxetine%20analog%29%20AND%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFMeNER%20OR%2018F-Reboxetine%20analog%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFMeNER%20OR%2018F-Reboxetine%20analog%29%20AND%20%28primate%20NOT%20human%29)]

Schou et al. (1) performed (S,S)-[^18^F]FMeNER-D_2_ PET imaging in two female cynomolgus monkeys. In each study, 49-68 MBq (1.3-1.8 mCi) of (S,S)-[^18^F]FMeNER-D_2_ was injected as a bolus. After injection at baseline conditions, the maximum activity in the monkey brain was ~3.6% of the total radioactivity 12 min after administration. The radioactivity was highest in the temporal cortex and lowest in the striatum. An equilibrium specific binding peak of the whole brain was observed between 120 and 160 min. The equilibrium specific binding peak was achieved in about 150 min in the temporal cortex. At 160 min, the region/striatum ratios were 1.5, 1.6, 1.3, and 1.5 for the lower brainstem, mesencephalon, thalamus, and temporal cortex, respectively. In comparison, (S,S)-[^18^F]FMeNER injection revealed skull-bound radioactivity that contaminated the brain images because of in vivo defluorination. Pretreatment with 5 mg/kg desipramine 20 min before (S,S)-[^18^F]FMeNER-D_2_ injection blocked radioactivity uptake in all regions. HPLC analysis of plasma samples showed that 85 ± 3% (n = 4) of (S,S)-[^18^F]FMeNER-D_2_ remained unchanged at 45 min and 76 ± 6% (n = 3) at 90 min.

Seneca et al. (2) reported whole-body distribution and radiation dosimetry of (S,S)-[^18^F]FMeNER-D_2_ in two female cynomolgus monkeys. The monkeys received doses of 65 MBq (1.8 mCi) and 76.4 MBq (2.1 mCi). The peak percentages of injected dose (% ID) in the lungs, kidneys, brain, liver, red bone marrow, heart, and urinary bladder were 26.8, 13.6, 5.7, 7.2, 5.0, 2.4, and 23% ID at peak times 1.42, 2.18, 4.48, 2, 2.06, 1.42, and 250 min, respectively. The cumulative urine excretion was 20.8% ID at 150 min. The effective t_½_ in the bladder was 0.649 h. The liver also showed rapid elimination with about two thirds of the liver radioactivity going to the gastrointestinal tract during the first 4 h. Calculations performed with the MIRDOSE 3.1 program indicated that the kidney was the critical organ, with 126 μGy/MBq (468 mrad/mCi), based on 2.4 h voiding intervals. The other organs with relatively higher doses (2.4 h voiding intervals) were the urinary bladder wall (114 μGy/MBq (422 mrad/mCi)), the heart wall (108 μGy/MBq (399 mrad/mCi)), the lungs (88.4 μGy/MBq (327 mrad/mCi)), the liver (28.3 μGy/MBq (105 mrad/mCi)), the upper large intestine (28.1 μGy/MBq (104 mrad/mCi)), the brain (27.6 μGy/MBq (102 mrad/mCi)), the small intestine 26.2 μGy/MBq (96.8 mrad/mCi)), and the bone marrow (22.2 μGy/MBq (82 mrad/mCi)).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B18F%5DFMeNER%20OR%2018F-Reboxetine%20analog%29%20AND%20human)]

No publication is currently available.

## NIH Support

NIN Intramural Support, KI(Karolinska Institutet)-NIH Graduate Training Partnership.

## References

1 Schou M., Halldin C., Sovago J., Pike V.W., Hall H., Gulyas B., Mozley P.D., Dobson D., Shchukin E., Innis R.B., Farde L. (2004). PET evaluation of novel radiofluorinated reboxetine analogs as norepinephrine transporter probes in the monkey brain. Synapse.
2 Seneca N., Andree B., Sjoholm N., Schou M., Pauli S., Mozley P.D., Stubbs J.B., Liow J.S., Sovago J., Gulyas B., Innis R., Halldin C. (2005). Whole-body biodistribution, radiation dosimetry estimates for the PET norepinephrine transporter probe (S,S)-[18F]FMeNER-D2 in non-human primates. Nucl Med Commun.
3 Konishi, J., B.A. Dwamena, M.D. Gross, B. Shapiro, T. Misaki, M. Fukunaga, J.C. Sisson, H.-Y. Oei, M. De Jong, and E. P. Krenning Endocrinology, in Molecular Nuclear Medicine, L.E. Feinendegen, W.W. Shreeve, W.C. Eckelman, Y.-W. Bahk, and H.N. Wagner Jr., Editor. 2003, Springer: New York. p. 357-409.
4 Antoni, G., T. Kihlberg, and B. Langstrom, Aspects on the synthesis of 11C-Labelled compounds, in Handbook of Radiopharmaceuticals, M.J. Welch, and C.S. Redvanly, Editor. 2003, John Wiley & Sons Ltd.: West Sussex, England. p. 141-194.
5 Sunderland, P.M., Pathophysiology. The Biologic basis for disease in adults and children, K.L. McCance, and S. E. Huether, Editor. 1994, Mosby-Year Books, Inc.: St, Louiis. p. 397-436.
6 Frey, K.A., PET study of neurochemical systems, in Positron Emission Tomography, P.E. Valk, D.L. Bailey, D.W. Townsend, and M.N. Maisey, Editors. 2002, Springer London. p. 309-327.
7 Buursma A.R., Beerens A.M., de Vries E.F., van Waarde A., Rots M.G., Hospers G.A., Vaalburg W., Haisma H.J. (2005). The Human Norepinephrine Transporter in Combination with 11C-m-Hydroxyephedrine as a Reporter Gene/Reporter Probe for PET of Gene Therapy. J Nucl Med.
8 Zahniser N.R., Doolen S. (2001). Chronic and acute regulation of Na+/Cl- -dependent neurotransmitter transporters: drugs, substrates, presynaptic receptors, and signaling systems. Pharmacol Ther.
9 Wilson A.A., Johnson D.P., Mozley D., Hussey D., Ginovart N., Nobrega J., Garcia A., Meyer J., Houle S. (2003). Synthesis and in vivo evaluation of novel radiotracers for the in vivo imaging of the norepinephrine transporter. Nucl Med Biol.
10 Langer O., Halldin C. (2002). PET and SPET tracers for mapping the cardiac nervous system. Eur J Nucl Med Mol Imaging.
11 Ding Y.S., Lin K.S., Logan J., Benveniste H., Carter P. (2005). Comparative evaluation of positron emission tomography radiotracers for imaging the norepinephrine transporter: (S,S) and (R,R) enantiomers of reboxetine analogs ([11C]methylreboxetine, 3-Cl-[11C]methylreboxetine and [18F]fluororeboxetine), (R)-[11C]nisoxetine, [11C]oxaprotiline and [11C]lortalamine. J Neurochem.
12 Iwata R., Pascali C., Bogni A., Furumoto S., Terasaki K., Yanai K. (2002). [18F]fluoromethyl triflate, a novel and reactive [18F]fluoromethylating agent: preparation and application to the on-column preparation of [18F]fluorocholine. Appl Radiat Isot.
13 Schou M., Halldin C., Pike V.W., Mozley P.D., Dobson D., Innis R.B., Farde L., Hall H. (2005). Post-mortem human brain autoradiography of the norepinephrine transporter using (S,S)-[18F]FMeNER-D2. Eur Neuropsychopharmacol.